# ^99m^Tc-Type II tumor necrosis receptor-Fc-interlukin-1 receptor antagonist fusion protein

Chemical name: | ^99m^Tc-Type II tumor necrosis receptor-Fc-interlukin-1 receptor antagonist fusion protein
Abbreviated name: | ^99m^Tc-TNFR2-Fc-IL-1ra
Synonym:
Agent category: | Polypeptide
Target: | Type II tumor necrosis receptor (TNFR2) and IL-1 receptors
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/protein/BAA89054.1), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NM_001066.2) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/gene/7133) for more information about the TNFR2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TNFR2-Fc-IL-1ra)]

Tumor necrosis factor (TNF) is a proinflammatory cytokine produced by macrophages, and it plays an important role in inflammation and immune response (1). There are two types of TNF (TNF-α, TNF-β). TNF-α is mainly responsible for initiating inflammatory responses by induction of several proinflammatory cytokines, chemokines, matrix metalloproteinases, and vascular endothelial adhesion molecules that attract leukocytes known to promote inflammation. There are two types of TNF receptors: TNFR1 and TNFR2. Soluble forms of TNF receptors are released upon proteolytic cleavage of the membrane-bound TNF receptors. Soluble TNF receptors participate in limiting the availability of TNF to bind to its receptors (2, 3). Several anti-TNF monoclonal antibodies (TNF blockers (http://www.fda.gov/Drugs/DrugSafety/PostmarketDrugSafetyInformationforPatientsandProviders/ucm109340.htm)) to further reduce circulating TNF have been approved by the United States Food and Drug Administration (FDA) for the treatment of a variety of inflammatory diseases (4, 5).

The interleukin-1 family consists of two proinflammatory cytokines, IL-1α and IL-1β, which bind to two IL-1 receptors (IL-1R1 and IL-1R2), and an IL-1R antagonist (IL-1ra), which is mainly produced by activated macrophages and tissue macrophages (6). IL-1α and IL-1β are important mediators of the inflammatory response and hematopoiesis, and they are involved in a variety of cellular activities, including cell proliferation, differentiation, and apoptosis. IL-1 is involved in chronic inflammatory diseases and in neuropathological conditions (7, 8). The balancing act of IL-1 and IL-1ra plays an important role in the regulation of inflammation and immune responses (9). IL-1ra has been shown to be effective as an anti-inflammatory treatment in several chronic inflammatory diseases and stroke (10, 11). A human recombinant, non-glycosylated form of the human IL-1ra (rhIL-1ra, Anakinra (http://google2.fda.gov/search?q=anakinra&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1&requiredfields=-archive%3AYes)) has been approved by the FDA for the treatment of rheumatoid arthritis (12).

IL-1β and TNF-α exhibit additive or synergistic effects in promoting pathophysiological processes observed in many inflammatory diseases (13). A dual domain TNFR2-Fc-IL-1ra fusion protein was constructed by joining TNFR2 and IL-1ra cDNA to the Fc fragment of human IgG_1_ cDNA in an expression plasmid (14). The amino-terminal segment binds to TNF, and the carboxyl-terminal sequence binds to the IL-1R. Liu et al. (14) radiolabeled TNFR2-Fc-IL-1ra with ^99m^Tc via 2-iminothiolane reduction to produce ^99m^Tc-TNFR2-Fc-IL-1ra for use with single-photon emission computed tomography (SPECT) imaging of inflammation in mice.

### Related Resource Links:

- Chapters in MICAD (IL-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=IL-1%20%5BAll+Fields%5D+AND+micad%5Bbook%5D), TNF (http://www.ncbi.nlm.nih.gov/books/?term=TNF+%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (IL-1á (http://www.ncbi.nlm.nih.gov/gene/3552), IL-1â (http://www.ncbi.nlm.nih.gov/gene/3553), IL-1R1 (http://www.ncbi.nlm.nih.gov/gene/3554), IL-1R2 (http://www.ncbi.nlm.nih.gov/gene/7850), IL-1ra (http://www.ncbi.nlm.nih.gov/gene/3557), TNF-α (http://www.ncbi.nlm.nih.gov/gene/7124), TNFR1 (http://www.ncbi.nlm.nih.gov/gene/21937), TNFR2 (http://www.ncbi.nlm.nih.gov/gene/7133))
- Articles in Online Mendelian Inheritance in Man (OMIM) (IL-1á (http://omim.org/entry/147760), IL-1â (http://omim.org/entry/147720), IL-1R1 (http://omim.org/entry/147810), IL-1R2 (http://omim.org/entry/147811), IL-1ra (http://omim.org/entry/147679), TNF (http://omim.org/entry/191160), TNFR1 (http://omim.org/entry/191190), TNFR2 (http://omim.org/entry/191191))
- Clinical trials (IL-1 (http://www.clinicaltrials.gov/ct2/results?term=IL-1&Search=Search), IL-1ra (http://www.clinicaltrials.gov/ct2/results?term=il-1ra&Search=Search), Anakinra (http://www.clinicaltrials.gov/ct2/results?term=anakinra), TNF (http://www.clinicaltrials.gov/ct2/results?term=TNF))
- Drug information in FDA (Anakinra (http://google2.fda.gov/search?q=anakinra&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1&requiredfields=-archive%3AYes), TNF blockers (http://www.fda.gov/Drugs/DrugSafety/PostmarketDrugSafetyInformationforPatientsandProviders/ucm109340.htm))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TNFR2-Fc-IL-1ra+and+synthesis)]

Liu et al. (14) reported the synthesis of ^99m^Tc-TNFR2-Fc-IL-1ra. TNFR2-Fc-IL-1ra was incubated with 2-iminothiolane for 30 min at 37°C in phosphate-buffered saline (PBS, pH 7.4). A solution of 925–1,110 MBq (25–30 mCi) ^99m^TcO_4_− was added to a mixture of SnCl_2_ and glucoheptonic acid and incubated at room temperature for 5 min to produce ^99m^Tc-glucoheptonate, which was then incubated with the thiolated TNFR2-Fc-IL-1ra for 30 min at room temperature, with a radiolabel yield of >97%. ^99m^Tc-TNFR2-Fc-IL-1ra was purified on a PD-10 column, with >95% radiochemical purity. The specific activity was 979–1,161 MBq/nmol (26.5–31.4 mCi/nmol). ^99m^Tc-TNFR2-Fc-IL-1ra remained >95% intact for up to 5 h in both saline at room temperature and serum at 37°C. For comparison studies, ^99m^Tc-IL-1ra-Fc and ^99m^Tc-TNFR2-Fc were prepared similarly, with specific activities of 297–409 MBq/nmol (8.0–11.1 mCi/nmol) and 766–1,034 MBq/nmol (20.7–27.9 mCi/nmol), respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TNFR2-Fc-IL-1ra+AND+in+vitro)]

Liu et al. (14) showed that ^99m^Tc-TNFR2-Fc-IL-1ra remained >95% and ~90% at 6 h and 21 h in either saline at room temperature or rat serum at 37°C, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TNFR2-Fc-IL-1ra+AND+rodentia)]

Liu et al. (14) performed ex vivo biodistribution studies in normal rats (n = 5/group) at 3 h after intravenous injection of 130–204 MBq (3.5–5.5 mCi) ^99m^Tc-TNFR2-Fc-IL-1ra, ^99m^Tc-IL-1ra-Fc, or ^99m^Tc-TNFR2-Fc. The biodistribution patterns were similar for all three radioligands, with each agent showing the highest accumulation in the kidneys (3.79%–5.18% injected dose/gram (ID/g), followed by the liver (1.29%–1.43% ID/g), small intestine (1.24%–2.39% ID/g), spleen (0.46%–0.81% ID/g), lung (0.45%–0.65% ID/g), heart (0.21%–0.42% ID/g), and stomach (0.13%–0.67% ID/g). Low radioactivity levels (<0.2% ID/g) were found in the large intestine, skin, and muscle. Blood radioactivity of ^99m^Tc-IL-1ra-Fc (1.27 ± 0.15% ID/g) was significantly lower than that of ^99m^Tc-TNFR2-Fc-IL-1ra (2.07 ± 0.07) and ^99m^Tc-TNFR2-Fc (2.10 ± 0.03) (P < 0.05). ^99m^Tc-TNFR2-Fc-IL-1ra remained >96% intact in the plasma at 3 h after injection.

Liu et al. (14) performed SPECT imaging studies in mice with TPA-induced edema in the right ears (n = 3–5/group) at 3 h after intravenous injection of 130–167 MBq (3.5–4.5 mCi) ^99m^Tc-TNFR2-Fc-IL-1ra, ^99m^Tc-IL-1ra-Fc, or ^99m^Tc-TNFR2-Fc. The inflamed ears were clearly visualized, whereas the contralateral ears were almost invisible. There was less radioactive accumulation of ^99m^Tc-IL-1ra-Fc in the inflamed ears compared to the accumulation of ^99m^Tc-TNFR2-Fc-IL-1ra and ^99m^Tc-TNFR2-Fc. Pretreatment with excess corresponding unlabeled ligand 30 min before the tracer reduced the radioactivity level to that of the contralateral left ears. Ex vivo studies showed that the radioactivity level of ^99m^Tc-TNFR2-Fc-IL-1ra (7.81 ± 0.86% ID/g) in the inflamed ears was significantly higher than that of ^99m^Tc-IL-1ra-Fc (2.76 ± 0.20% ID/g) and ^99m^Tc-TNFR2-Fc (5.86 ± 0.40% ID/g) (P < 0.05), with inflamed ear/control ear ratios of 4.13, 4.78, and 2.31, respectively. Pretreatment with excess corresponding unlabeled ligand 30 min before the tracer reduced the ratios to 2.09, 2.32, and 1.69, respectively. The levels of IL-1β and TNF-α were significantly increased in the TPA-treated ears compared with contralateral ears (IL-1β: 424 ± 15 pg/mg protein versus 65 ± 21 pg/mg protein, P < 0.05; TNF-α: 33.7 ± 4.2 pg/mg protein versus 16.8 ± 1.3 pg/mg protein, P < 0.01).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TNFR2-Fc-IL-1ra+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TNFR2-Fc-IL-1ra+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TNFR2-Fc-IL-1ra+AND+human)]

No publication is currently available.

## NIH Support

R01 HL090716, P41 EB002035

## References

1 Jaattela M. (1991). Biologic activities and mechanisms of action of tumor necrosis factor-alpha/cachectin. Lab Invest.
2 Fernandez-Botran R., Crespo F.A., Sun X. (2002). Soluble cytokine receptors in biological therapy. Expert Opin Biol Ther.
3 Fernandez-Botran R. (2000). Soluble cytokine receptors: novel immunotherapeutic agents. Expert Opin Investig Drugs.
4 Behm B.W., Bickston S.J. (2008). Tumor necrosis factor-alpha antibody for maintenance of remission in Crohn's disease. Cochrane Database Syst Rev.
5 Danese S., Semeraro S., Armuzzi A., Papa A., Gasbarrini A. (2006). Biological therapies for inflammatory bowel disease: research drives clinics. Mini Rev Med Chem.
6 Dinarello C.A. (1996). Biologic basis for interleukin-1 in disease. Blood.
7 McColl B.W., Allan S.M., Rothwell N.J. (2009). Systemic infection, inflammation and acute ischemic stroke. Neuroscience.
8 Simi A., Tsakiri N., Wang P., Rothwell N.J. (2007). Interleukin-1 and inflammatory neurodegeneration. Biochem Soc Trans.
9 Dinarello C.A., Simon A., van der Meer J.W. (2012). Treating inflammation by blocking interleukin-1 in a broad spectrum of diseases. Nat Rev Drug Discov.
10 Neven B., Marvillet I., Terrada C., Ferster A., Boddaert N., Couloignier V., Pinto G., Pagnier A., Bodemer C., Bodaghi B., Tardieu M., Prieur A.M., Quartier P. (2010). Long-term efficacy of the interleukin-1 receptor antagonist anakinra in ten patients with neonatal-onset multisystem inflammatory disease/chronic infantile neurologic, cutaneous, articular syndrome. Arthritis Rheum.
11 Emsley H.C., Smith C.J., Georgiou R.F., Vail A., Hopkins S.J., Rothwell N.J., Tyrrell P.J. (2005). A randomised phase II study of interleukin-1 receptor antagonist in acute stroke patients. J Neurol Neurosurg Psychiatry.
12 Thompson R.C., Dripps D.J., Eisenberg S.P. (1992). Interleukin-1 receptor antagonist (IL-1ra) as a probe and as a treatment for IL-1 mediated disease. Int J Immunopharmacol.
13 Cain B.S., Meldrum D.R., Dinarello C.A., Meng X., Joo K.S., Banerjee A., Harken A.H. (1999). Tumor necrosis factor-alpha and interleukin-1beta synergistically depress human myocardial function. Crit Care Med.
14 Liu Z., Wyffels L., Barber C., Wan L., Xu H., Hui M.M., Furenlid L.R., Woolfenden J.M. (2012). Characterization of 99mTc-labeled cytokine ligands for inflammation imaging via TNF and IL-1 pathways. Nucl Med Biol.